# N-(4-(6-(Isopropylamino)pyrimidin-4-yl)-1,3-thiazol-2-yl)-4-[^11^C]methoxy-N-methylbenzamide

Chemical name: | N-(4-(6-(Isopropylamino)pyrimidin-4-yl)-1,3-thiazol-2-yl)-4-[^11^C]methoxy-N-methylbenzamide
Abbreviated name: | [^11^C]ITMM, [^11^C]6
Synonym:
Agent category: | Compound
Target: | Metabotropic glutamate receptor subtype 1 (mGluR1)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ITMM)]

Glutamate is a major excitatory neurotransmitter at neuronal synapses in the central nervous system (CNS) (1, 2). Glutamate produces excitatory effects by acting on cell-surface ionotropic glutamate or metabotropic glutamate receptors (mGluRs). The mGluRs are GTP-binding protein (G-protein)–coupled receptors that play important roles in regulating the activity of many synapses in the CNS, and many neuronal projection pathways contain mGluRs. There are eight mGluR subtypes, which are further subdivided into groups I, II, and III. The group I receptors include mGluR1 and mGluR5, and they are found predominantly in postsynaptic locations. mGluR1 is found in moderate to high density in the cerebellum, caudate, putamen, thalamus, cingulate cortex, and hippocampus, with low density in the pons. mGluR5 is usually found in moderate to high density in the frontal cortex, caudate, putamen, nucleus accumbens, olfactory tubercle, and hippocampus, with low density in the cerebellum. mGluR1 and mGluR5 are positively coupled to phospholipase C in the regulation of neuronal excitability (3). Dysfunction of mGluR1 and mGluR5 is implicated in a variety of diseases in the CNS, including anxiety, depression, schizophrenia, Parkinson’s disease, and drug addiction or withdrawal (2, 4).

Positron emission tomography (PET) radioligands targeting mGluR5 can visualize and analyze mGluR5 expression in normal physiological and pathological conditions (4-8). However, only a few mGluR1 ligands have been studied. N-(4-(6-(Isopropylamino)pyrimidin-4-yl)-1,3-thiazol-2-yl)-4-methoxy-N-methylbenzamide (ITMM) was shown to be a selective mGluR1 antagonist with nanomolar affinity (K_i_ = 12.6 nM), with little inhibition of mGluR5. Fujinaga et al. (9) labeled ITMM with ^11^C to prepare N-(4-(6-(isopropylamino)pyrimidin-4-yl)-1,3-thiazol-2-yl)-4-[^11^C]methoxy-N-methylbenzamide ([^11^C]ITMM) for use with in vivo PET imaging of mGluR1 distribution in rat brains. Toyohara et al. (10) evaluated [^11^C]ITMM in mouse and human brains. [^11^C]ITMM was shown to be a suitable PET radioligand for mapping mGluR1 in the human brain.

### Related Resource Links:

- Chapters in MICAD (mGluR1 (http://www.ncbi.nlm.nih.gov/books?Db=books&Cmd=DetailsSearch&Term=mGluR1+AND+micad%5Bbook%5D), mGluR5 (http://www.ncbi.nlm.nih.gov/books?term=mGluR5%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (mGluR1 (http://www.ncbi.nlm.nih.gov/gene/2911), mGluR5 (http://www.ncbi.nlm.nih.gov/gene/2915))
- Articles in Online Mendelian Inheritance in Man (OMIM) (mGluR1 (http://omim.org/entry/604473), mGluR5 (http://www.ncbi.nlm.nih.gov/omim/604102))
- Clinical trials (mGluR1 (http://www.clinicaltrials.gov/ct2/results?term=mGluR1), mGluR5 (http://www.clinicaltrials.gov/ct2/results?term=mglur5))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ITMM%20and%20synthesis)]

Fujinaga et al. (9) synthesized [^11^C]ITMM by methylation of the hydroxyl precursor with [^11^C]MeI (prepared with [^11^C]CO_2_) for 5 min at 70°C. Subsequent separation with high-performance liquid chromatography (HPLC) produced a radiochemical purity >99%. Average radiochemical yield was 22 ± 5% (n = 21) based on [^11^C]CO_2_. The specific activity of [^11^C]ITMM was 95–140 GBq/µmol (2.56–3.78 Ci/µmol) at the end of synthesis (EOS). The total synthesis time was 25 ± 3 min from the end of bombardment (EOB). For higher specific activity, [^11^C]ITMM was prepared via methylation of the hydroxyl precursor with [^11^C]MeI (prepared with [^11^C]CH_4_) for 5 min at 70°C. Average radiochemical yield was 6 ± 1% (n = 3) based on [^11^C]CH_4_. The specific activity of [^11^C]ITMM was 4,370–7,840 GBq/µmol (118–212 Ci/µmol) at EOS. The total synthesis time was 29 ± 1 min.

Toyohara et al. (10) prepared [^11^C]ITMM by methylation of the hydroxyl precursor with [^11^C]methyl triflate under NaOH as a base using an automated synthesizer for 1 min at room temperature. Subsequent separation with HPLC produced a radiochemical purity >98%. Average radiochemical yield was 66.0 ± 27.4% (n = 4) based on [^11^C]methyl triflate. The specific activity of [^11^C]ITMM was 97.9–351.1 GBq/µmol (2.64–9.49 Ci/µmol) at EOS. The total synthesis time was <25 min from the EOB.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ITMM%20and%20in%20vitro)]

In vitro binding affinity of ITMM was determined with rat brain homogenates using [^18^F]fluoro-N-[4-[6-(isopropylamino)pyrimidin-4-yl]-1,3-thiazol-2-yl]-N-methylbenzamide ([^18^F]FITM) as the mGluR1 radioligand (9). The K_i_ values were 12.6 ± 1.2 nM and 5.4 ± 1.2 nM for ITMM and FITM, respectively. Both agents showed IC_50_ values >10,000 nM for mGluR5. ITMM (LogD 2.57) was found to be more lipophilic than FITM (LogD 1.45).

In vitro [^11^C]ITMM autoradiographic imaging studies were performed on rat brain sections (9). [^11^C]ITMM bound heterogeneously to the brain sections, with the highest accumulation of radioactivity in the mGluR1-rich cerebellum, followed by the thalamus and striatum, with the lowest radioactivity in the pons. JNJ-16259685 (1,000 nM), another mGluR1 antagonist, blocked radioactivity signals by >70% in the cerebellum, thalamus, and striatum.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ITMM%20and%20rodentia)]

Fujinaga et al. (9) performed ex vivo biodistribution studies in mice (n = 4/group) at 1–60 min after intravenous injection of 4.8 MBq (0.13 mCi) [^11^C]ITMM (0.04 nmol). The radioactivity levels in most tissues were highest at 1–5 min and decreased gradually thereafter. The highest accumulation at 5 min was observed in the liver (8.34% injected dose/gram (ID/g)), followed by the kidney (5.64% ID/g), small intestine (4.55% ID/g), brain (3.21% ID/g), lung (2.90% ID/g), heart (2.09% ID/g), spleen (1.96% ID/g), blood (1.95% ID/g), and muscle (1.22% ID/g). The accumulation in the brain remained high at 2.38% ID/g and 1.85% ID/g at 30 min and 60 min, respectively.

Fujinaga et al. (9) performed dynamic PET imaging studies for 90 min in rats (n = 4) after intravenous injection of 37–55 MBq (1.0–1.5 mCi) [^11^C]ITMM (0.3–0.5 nmol). Blocking studies were performed with injection of excess ITMM (1 mg/kg) or mGluR1 antagonist JNJ-16259685 (3 mg/kg) just before injection of the tracer. Baseline tissue time-activity curves revealed high accumulation of radioactivity that peaked at 30–45 min in the cerebellum, with moderate radioactivity in the thalamus and striatum and low radioactivity in the pons. The cerebellum/pons, thalamus/pons, and striatum/pons maximum ratios were 6.98, 5.05, and 4.32, respectively. Both ITMM and JNJ-16259685 showed >85% inhibition of radioactivity in the cerebellum, thalamus, and striatum. PET imaging studies with wild-type and mGluR1-knockout mice showed high radioactivity in the cerebellum and thalamus in the wild-type mouse brain and only a low, homogeneous distribution of radioactivity in the knockout mouse brain. Toyohara et al. (10) showed that the maximum standard uptake values in the cerebellum, cerebral cortex, and striatum were 1.7, 0.9, and 0.8, respectively, at 15 min after injection of [^11^C]ITMM in mice (n = 4).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ITMM%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ITMM%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ITMM%20and%20human)]

Toyohara et al. (10) performed dynamic PET imaging scans for 90 min with a normal male subject (27 years old) after injection of 565 MBq (15.3 mCi) [^11^C]ITMM (8 nmol). Radioactivity in the cerebellum reached a plateau at 40 min. The volume of distribution (V_T_) values were 2.7, 1.1, 0.9, 0.8, 0.7, 0.6, 0.5, and 0.5 for the cerebellum, thalamus, temporal cortex, parietal cortex, frontal cortex, occipital cortex, caudate, and putamen, respectively. [^11^C]ITMM remained 84.7% intact in the blood at 10 min and declined to 60.5% intact at 60 min. Plasma radioactivity decreased rapidly and exhibited a three-phase clearance pattern with half-lives of 1, 4, and 29 min.

## References

1 Pin J.P., Duvoisin R. (1995). The metabotropic glutamate receptors: structure and functions. Neuropharmacology.
2 Ferraguti F., Crepaldi L., Nicoletti F. (2008). Metabotropic glutamate 1 receptor: current concepts and perspectives. Pharmacol Rev.
3 Abe T., Sugihara H., Nawa H., Shigemoto R., Mizuno N., Nakanishi S. (1992). Molecular characterization of a novel metabotropic glutamate receptor mGluR5 coupled to inositol phosphate/Ca2+ signal transduction. J Biol Chem.
4 Gasparini F., Lingenhohl K., Stoehr N., Flor P.J., Heinrich M., Vranesic I., Biollaz M., Allgeier H., Heckendorn R., Urwyler S., Varney M.A., Johnson E.C., Hess S.D., Rao S.P., Sacaan A.I., Santori E.M., Velicelebi G., Kuhn R. (1999). 2-Methyl-6-(phenylethynyl)-pyridine (MPEP), a potent, selective and systemically active mGlu5 receptor antagonist. Neuropharmacology.
5 Ametamey S.M., Kessler L.J., Honer M., Wyss M.T., Buck A., Hintermann S., Auberson Y.P., Gasparini F., Schubiger P.A. (2006). Radiosynthesis and preclinical evaluation of 11C-ABP688 as a probe for imaging the metabotropic glutamate receptor subtype 5. J Nucl Med.
6 Ametamey S.M., Treyer V., Streffer J., Wyss M.T., Schmidt M., Blagoev M., Hintermann S., Auberson Y., Gasparini F., Fischer U.C., Buck A. (2007). Human PET studies of metabotropic glutamate receptor subtype 5 with 11C-ABP688. J Nucl Med.
7 Baumann C.A., Mu L., Johannsen S., Honer M., Schubiger P.A., Ametamey S.M. (2010). Structure-activity relationships of fluorinated (E)-3-((6-methylpyridin-2-yl)ethynyl)cyclohex-2-enone-O-methyloxime (ABP688) derivatives and the discovery of a high affinity analogue as a potential candidate for imaging metabotropic glutamate recepors subtype 5 (mGluR5) with positron emission tomography (PET). J Med Chem.
8 Honer M., Stoffel A., Kessler L.J., Schubiger P.A., Ametamey S.M. (2007). Radiolabeling and in vitro and in vivo evaluation of [(18)F]-FE-DABP688 as a PET radioligand for the metabotropic glutamate receptor subtype 5. Nucl Med Biol.
9 Fujinaga M., Yamasaki T., Yui J., Hatori A., Xie L., Kawamura K., Asagawa C., Kumata K., Yoshida Y., Ogawa M., Nengaki N., Fukumura T., Zhang M.R. (2012). Synthesis and evaluation of novel radioligands for positron emission tomography imaging of metabotropic glutamate receptor subtype 1 (mGluR1) in rodent brain. J Med Chem.
10 Toyohara J., Sakata M., Fujinaga M., Yamasaki T., Oda K., Ishii K., Zhang M.R., Moriguchi Jeckel C.M., Ishiwata K. (2013). Preclinical and the first clinical studies on [(11)C]ITMM for mapping metabotropic glutamate receptor subtype 1 by positron emission tomography. Nucl Med Biol.